# 6-[1-(2-[^18^F]Fluoro-3-pyridyl)-5-methyl-1H-1,2,3-triazol-4-yl]quinoline

Chemical name: | 6-[1-(2-[^18^F]Fluoro-3-pyridyl)-5-methyl-1H-1,2,3-triazol-4-yl]quinoline
Abbreviated name: | [^18^F]FPTQ, [^18^F]7a
Synonym:
Agent category: | Compound
Target: | Metabotropic glutamate receptor subtype 1 (mGluR1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FPTQ)]

Glutamate is a major excitatory neurotransmitter at neuronal synapses in the central nervous system (CNS) (1, 2). Glutamate produces its excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate receptors (mGluRs). The mGluRs are GTP-binding protein (G-protein)–coupled receptors that play important roles in regulating the activity of many synapses in the CNS, and many neuronal projection pathways contain mGluRs. There are eight mGluR subtypes, which are further subdivided into groups I, II, and III. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. The mGluR1 is found in moderate to high density in the cerebellum, caudate, putamen, thalamus, cingulate cortex, and hippocampus, with low density in the pons. The mGluR5 is usually found in moderate to high density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, and hippocampus, whereas the density in the cerebellum is low. The mGluR1 and mGluR5 are positively coupled to phospholipase C in the regulation of neuronal excitability (3). Dysfunction of mGluR1 and mGluR5 is implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal (2, 4).

Positron emission tomography (PET) and single-photon emission tomography of radioligands targeting mGluR1 can visualize and analyze mGluR1 expression in normal physiological and pathological conditions. Several radioligands have been studied for in vivo imaging of mGluR1 in the brain (5). 6-[1-(2-(Fluoro-3-pyridyl)-5-methyl-1H-1,2,3-triazol-4-yl]quinoline (FPTQ) was shown to be a selective mGluR1 with nanomolar affinity (3.6 nM), with little inhibition to mGluR5 (6). Fujinaga et al. (7) prepared and evaluated 6-[1-(2-[^18^F] fluoro-3-pyridyl)-5-methyl-1H-1,2,3-triazol-4-yl]quinoline ([^18^F]FPTQ) for use with in vivo PET imaging of mGluR1 distribution in rats. The investigators concluded that [^18^F]FPTQ is not suitable for PET imaging of GluR1 in the brain because of its rapid dissociation and the presence of radiolabeled metabolite in the brain.

### Related Resource Links:

- Chapters in MICAD (mGluR1 (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=mGluR1+AND+micad%5Bbook%5D), mGluR5 (http://www.ncbi.nlm.nih.gov/books?term=mGluR5%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (mGluR1 (http://www.ncbi.nlm.nih.gov/gene/2911), mGluR5 (http://www.ncbi.nlm.nih.gov/gene/2915))
- Articles in Online Mendelian Inheritance in Man (OMIM) (mGluR1 (http://omim.org/entry/604473), mGluR5 (http://www.ncbi.nlm.nih.gov/omim/604102))
- Clinical trials (mGluR1 (http://www.clinicaltrials.gov/ct2/results?term=mGluR1), mGluR5 (http://www.clinicaltrials.gov/ct2/results?term=mglur5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTQ%20and%20synthesis)]

Fujinaga et al. (7) reported a one-step automated synthesis of [^18^F]FPTQ. The bromo-precursor was subjected to nucleophilic fluorination with K[^18^F]F for 10 min at 150°C, with a radiochemical yield of 69 ± 13% and an average specific activity of 118–237 GBq/µmol (3.2–6.4 Ci/µmol, n = 8) at the end of synthesis. The radiochemical purity of [^18^F]FPTQ was >99% after purification with high-performance liquid chromatography. The total synthesis time was 75 min. [^18^F]FPTQ exhibited a Log D value of 2.53 ± 0.02 (n = 3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTQ%20and%20in%20vitro)]

In vitro [^18^F]FPTQ autoradiographic imaging studies were performed on brain sections of rats (n = 4) (7). [^18^F]FPTQ bound heterogeneously to the brain sections, with the highest accumulation of radioactivity in the mGluR1-rich cerebellum (408.8 ± 48.1 PSL/mm^2^), followed by the thalamus (188.9 ± 44.4 PSL/mm^2^), hippocampus (112.4 ± 29.4 PSL/mm^2^), striatum (70.7 ± 14.2 PSL/mm^2^), cerebral cortex (28.2 ± 4.7 PSL/mm^2^), and pons (17.5 ± 2.7 PSL/mm^2^). FPTQ and JNJ-16259685 (1,000 nM, mGluR1 antagonists) completely blocked radioactive signals to background levels in these brain regions. On the other hand, the mGluR5 antagonist MPEP (1,000 nM) demonstrated only marginal inhibition (~10%) of the signals.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTQ%20and%20rodentia)]

Fujinaga et al. (7) performed ex vivo biodistribution studies in rats (n = 3/group) at 5, 15, and 30 min after intravenous injection of 17 MBq (0.46 mCi) [^18^F]FPTQ (0.11 nmol). The radioactivity levels in most tissues were highest at 5 min and decreased quickly thereafter. The highest accumulation at 5 min was observed in the small intestine (3.1% injected dose/gram (ID/g)), followed by the liver (2.3% ID/g), kidney (0.76% ID/g), pancreas (0.75% ID/g), brain (0.52% ID/g), lung (0.50% ID/g), heart (0.47% ID/g), spleen (0.43% ID/g), blood (0.38% ID/g), muscle (0.28% ID/g), and bone (0.22% ID/g). [^18^F]FPTQ bound heterogeneously to the brain sections, with the highest accumulation of radioactivity at 5 min in the mGluR1-rich cerebellum (1.21% ID/g) and thalamus (0.73% ID/g), followed by the hippocampus (0.58% ID/g), striatum (0.54% ID/g), pons-medulla (0.47% ID/g), and cerebral cortex (0.44% ID/g). However, the accumulation levels in the cerebellum and the rest of the brain regions were 0.20% ID/g and 0.10% ID/g at 30 min, respectively.

Fujinaga et al. (7) performed dynamic PET imaging studies for 60 min in rats (n = 4/group) after intravenous injection of 17.5 MBq (0.5 mCi) [^18^F]FPTQ. Blocking studies were performed by pretreatment (0.5 min) with 1 mg/kg FPTQ, JNJ-16259685, or MPEP. Baseline tissue time-activity curves revealed a high accumulation of radioactivity at 1–3 min in the cerebellum (standard uptake value (SUV) = 2.3), followed by the thalamus (2.1), striatum (1.8), hippocampus (1.6), and cerebral cortex (1.5), whereas little radioactivity was detected in the medulla (1.1). The radioactivity levels of all brain regions decreased faster than that of the cerebellum after the initial accumulation. The cerebellum/medulla, thalamus/medulla, striatum/medulla, hippocampus/medulla, and cerebral cortex/medulla ratios at 10–15 min were 3.73, 1.91, 1.55, 1.42, and 1.31, respectively. Pretreatment with FPTQ or JNJ-16259685 reduced the radioactivity signals to background level, whereas pretreatment with MPEP showed little inhibition.

Ex vivo metabolite studies were performed in mice (n = 3/group) at 5–30 min after intravenous injection of [^18^F]FPTQ (7). [^18^F]FPTQ remained 4% intact in the plasma at 30 min with one polar metabolite. On the other hand, [^18^F]FPTQ remained 67% and 34% intact at 30 min in the cerebellum and brain minus cerebellum, respectively. The investigators concluded that [^18^F]FPTQ is not suitable for PET imaging of GluR1 in the brain because of the rapid dissociation and the presence of radiolabeled metabolite in the brain.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTQ%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTQ%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPTQ%20and%20human)]

No publication is currently available.

## References

1 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
2 Ferraguti F., Crepaldi L., Nicoletti F. (2008). Metabotropic glutamate 1 receptor: current concepts and perspectives. Pharmacol Rev.
3 Abe T., Sugihara H., Nawa H., Shigemoto R., Mizuno N., Nakanishi S. (1992). Molecular characterization of a novel metabotropic glutamate receptor mGluR5 coupled to inositol phosphate/Ca2+ signal transduction. J Biol Chem.
4 Gasparini F., Lingenhohl K., Stoehr N., Flor P.J., Heinrich M., Vranesic I., Biollaz M., Allgeier H., Heckendorn R., Urwyler S., Varney M.A., Johnson E.C., Hess S.D., Rao S.P., Sacaan A.I., Santori E.M., Velicelebi G., Kuhn R. (1999). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP), a potent, selective and systemically active mGlu5 receptor antagonist. Neuropharmacology.
5 Yamasaki T., Fujinaga M., Yoshida Y., Kumata K., Yui J., Kawamura K., Hatori A., Fukumura T., Zhang M.R. (2011). Radiosynthesis and preliminary evaluation of 4-[18F]fluoro-N-[4-[6-(isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methylb enzamide as a new positron emission tomography ligand for metabotropic glutamate receptor subtype 1. Bioorg Med Chem Lett.
6 Suzuki G., Kawagoe-Takaki H., Inoue T., Kimura T., Hikichi H., Murai T., Satow A., Hata M., Maehara S., Ito S., Kawamoto H., Ozaki S., Ohta H. (2009). Correlation of receptor occupancy of metabotropic glutamate receptor subtype 1 (mGluR1) in mouse brain with in vivo activity of allosteric mGluR1 antagonists. J Pharmacol Sci.
7 Fujinaga M., Yamasaki T., Kawamura K., Kumata K., Hatori A., Yui J., Yanamoto K., Yoshida Y., Ogawa M., Nengaki N., Maeda J., Fukumura T., Zhang M.R. (2011). Synthesis and evaluation of 6-[1-(2-[(18)F]fluoro-3-pyridyl)-5-methyl-1H-1,2,3-triazol-4-yl]quinoline for positron emission tomography imaging of the metabotropic glutamate receptor type 1 in brain. Bioorg Med Chem.